# N-[2-(4-[^18^F]Fluorobenzamido)ethyl]maleimide-sulfhydryl-cyclic-arginine-glycine-aspartic acid peptide

Chemical name: | N-[2-(4-[^18^F]Fluorobenzamido)ethyl]maleimide-sulfhydryl-cyclic-arginine-glycine-aspartic acid peptide
Abbreviated name: | [^18^F]FBEM-SRGD
Synonym: | ^18^F-RGD
Agent Category: | Peptide
Target: | Integrin α_v_β_3_
Target Category: | Receptor binding
Method of detection: | Positron Emission Tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov). Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4504763), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=40217844) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3685) for more information about integrin α_v_β_3_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F-RGD+OR+(18F-labeled+PEGylated+RGD+peptide)&WebEnv=0BLLjNep_4Na8W4oAlg1o8IYrXYJs6c8bHcZcM1npsIX2eqMoFrtJDI8lZfqNqMd47xB9b-jfArvt%40D4664A2364C62360_0155SID&WebEnvRq=1)]

N-[2-(4-[^18^F]Fluorobenzamido)ethyl]maleimide-sulfhydryl-cyclic-arginine-glycine-aspartic acid peptide ([^18^F]FBEM-SRGD) is an integrin-targeted molecular imaging agent developed for positron emission tomography (PET) of tumor vasculature and angiogenesis (1). ^18^F is a positron emitter with a physical half-life (t_½_) of 110 min.

Cellular survival, invasion, and migration control embryonic development, angiogenesis, tumor metastasis, and other physiological processes (2, 3). Among the molecules that regulate angiogenesis are integrins, which comprise a superfamily of cell adhesion proteins that form heterodimeric receptors for extracellular matrix (ECM) molecules (4, 5). These transmembrane glycoproteins consist of two noncovalently associated subunits, α and β (18 α- and 8 β-subunits in mammals), which are assembled into at least 24 α/β pairs. Several integrins, such as integrin α_v_β_3_, have affinity for the arginine-glycine-aspartic acid (RGD) tripeptide motif, which is found in many ECM proteins. Expression of integrin α_v_β_3_ receptors on endothelial cells is stimulated by angiogenic factors and environments. The integrin α_v_β_3_ receptor is generally not found in normal tissue, but it is strongly expressed in vessels with increased angiogenesis. It is significantly upregulated in certain types of tumor cells and in almost all tumor vasculature.

Molecular imaging probes carrying the RGD motif that binds to the integrin α_v_β_3_ can be used to image tumor vasculature and evaluate angiogenic response to tumor therapy (6, 7). Various RGD peptides in both linear and cyclic forms have been developed for in vivo binding to integrin α_v_β_3_ (8). Chen et al. (9) evaluated ^64^Cu-labeled and 18F-labeled cyclic RGD peptide [c(RGDyK)] monomers in nude mice bearing breast tumors. [^18^F]FB-c(RGDyK) showed high tumor accumulation but also rapid tumor washout with unfavorable biliary excretion (10). To improve the pharmacokinetics and tumor retention of the radiolabeled peptide, a dimer analog was synthesized as [^18^F]FB-[c(RGDyK)]_2_, which showed improved tumor localization and predominant renal excretion (11). Radiofluorination can generally be achieved through the functional groups of amino, carboxylic acid, and sulfhydryl. Labeling of RGD peptide with ^18^F in most fluorinated peptide studies used ^18^F-synthons such as N-succinimidyl 4-[^18^F]fluorobenzoate to form a stable amide bond by reacting with primary amino groups of RGD peptides at the N terminus or the lysine side chain (1). One of the main concerns with this approach is the potential interference with the biological activities of these peptides. Cai et al. (1) suggested that ^18^F-labeling of RGD peptides via the carboxylic acid group at the C terminus or internal glutamic/aspartic acid side chain might minimize the potential interference. They reported the use of a thiol-reactive ^18^F-synthon, ^18^F-FBEM, as the prosthetic group for labeling a sulfhydryl-functionalized c(RGDyK) monomeric peptide (SRGD) and a E[c(RGDyK)]_2_ dimeric peptide (SRGD2). The maleimide group in ^18^F-FBEM allows for a thiol-specific Michael addition reaction.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(18F-RGD+OR+(18F-labeled+PEGylated+RGD+peptide))+AND+synthesis&WebEnv=0I2bF98RYiQ70qDnPf_X9WlKizvFUUDnAUh7lSB_Vxc4SgCntBxAI7WmGjhsZce-S9o1O_eYPQl6Z%40D4664A2364C62360_0155SID&WebEnvR)]

The c(RGDyK) peptide was first prepared via solution cyclization of the fully protected linear pentapeptide H-Gly-Asp(OtBu)-D-Tyr(OtBu)-Lys(Boc)-Arg(Pbf)-OH, followed by deprotection with trifluoroacetic acid (TFA) in the presence of the free radical scavenger triisopropylsilane (1, 12). The c(RGDyK) was conjugated to N-succinimidyl S-acetylthioacetate (SATA) by mixing c(RGDyK) in sodium borate (Na_2_B_4_O_7_) buffer (pH 8.5) with SATA in dimethyl sulfoxide (1). The yield was 95%. The crude SATA-c(RGDyK) was then dissolved in water and mixed with L-hydroxylamine (pH 6.0) for 2 h to yield the SRGD. The final product was purified with semi-preparative high-performance liquid chromatography (HPLC). The overall yield was 80%. The identity of the SRGD peptide (C_29_H_43_N_9_O_9_S) was confirmed by matrix-assisted laser desorption/ionization time-of-flight mass spectroscopy. FBEM was obtained by reacting N-(2-aminoethyl)maleimide with N-succinimidyl 4-fluorobenzoate in Na_2_B_4_O_7_ (pH 8.5) at 50ºC for 20 min. The reaction was quenched with 2% TFA. The yield was 85% after HPLC purification.

Cai et al. (1) reported the radiolabeling of [^18^F]FBEM-SRGD with the use of [^18^F]FBEM, which was first prepared from N-succinimidyl 4-[^18^F]fluorobenzoate ([^18^F]SFB) (10, 13). Then [^18^F]SFB in acetonitrile was mixed with N-(2-aminoethyl)maleimide and N,N-diisopropylethylamine. The reaction mixture was heated at 40ºC for 20 min and then quenched with TFA. The HPLC-purified [^18^F]FBEM was obtained with a total reaction time of 150 ± 20 min. The non–decay-corrected radiochemical yield was 5 ± 2% (on the basis of ^18^F-F−) with a specific activity of 150–200 TBq/mmol (4,050–5,400 Ci/mmol). Purified [^18^F]FBEM in phosphate-buffered saline was mixed with the SRGD peptide in dimethyl sulfoxide and tris(2-carboxyethyl)phosphine hydrochloride in water. The pH of the mixture was adjusted to 7.0–7.5 and incubated at room temperature for 20 min. The resulting [^18^F]FBEM-SRGD was purified with HPLC. The radiochemical yield was 85 ± 5% (non–decay-corrected) on the basis of [^18^F]FBEM. The total reaction time, including final HPLC purification, was ~200 ± 25 min. The overall decay-corrected radiochemical yield was 20 ± 4% (n = 5), and the specific activity was 100–150 TBq/mmol (2,700–4,050 Ci/mmol). The radiochemical purity was >98%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F-RGD+OR+(18F-labeled+PEGylated+RGD+peptide))+AND+in+vitro&WebEnv=0a5II5Gs_JOpUmsnQikbvuPGARlXBgKwCgwH9GaXPnG-a7NAOoYeqYwolMM4vvyMkqFnISiJ3cZsp%40D4664A2364C62360_0155SID&WebEnvRq=)]

Cai et al. (1) determined the octanol/water partition coefficient (Log P) of [^18^F]FBEM-SRGD to be 0.93 ± 0.02. In vitro cell-binding affinity studies of the unlabeled FBEM-SRGD was conducted in U87MG glioblastoma cells with ^125^I-echistatin as the integrin α_v_β_3_–specific radioligand. The inhibition concentration (IC_50_) for FBEM-SRGD was determined to be 66.8 ± 5.1 nM. In comparison, the IC_50_ for c(RGDyK) was determined to be 51.3 ± 4.2 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(18F-RGD+OR+(18F-labeled+PEGylated+RGD+peptide))+AND+rodentia&WebEnv=0f8W2adxgufdPEvIqGnB3mHoFAaNf1vIR3nXXc8cwSwi7exEDpOXWAccr9Zfy1_6f9cwG471xstYC%40D4664A2364C62360_0155SID&WebEnvRq)]

Biodistribution studies of [^18^F]FBEM-SRGD were conducted in nude mice bearing the U87MG glioblastoma on the right front leg and the MDA-MB-435 breast cancer carcinoma on the left mammary fat pad (1). Both tumor volumes reached ~30–400 mm^3^. Each mouse received 1 MBq (27 μCi) of [^18^F]FBEM-SRGD by i.v. administration. At 60 min, the radioactivity levels (n = 3) in percentage of injected dose per gram (% ID/g) detected in the U87MG and MDA-MB-435 tumors were 1.33 ± 0.28 and 1.43 ± 0.11, respectively. In comparison, the radioactivity levels in the U87MG and MDA-MB-435 tumors for the dimeric [^18^F]FBEM-SRGD2 were 2.71 ± 0.19% ID/g and 5.25 ± 0.17% ID/g, respectively. When blocked by coinjection of 10 mg/kg c(RGDyK), these levels decreased to 0.40 ± 0.02% ID/g (P < 0.05) and 0.77 ± 0.04% ID/g (P < 0.05), respectively. [^18^F]FBEM-SRGD was relatively hydrophobic and exhibited high hepatobiliary excretion. By extrapolation from Figure 3 of the article by Cai et al. (1), the radioactivity levels at 10 min were estimated to be ~3% ID/g, ~10% ID/g, ~9% ID/g, and ~2% ID/g for the blood, liver, kidney, and intestine, respectively. At 60 min, these levels appeared to change to ~0.2% ID/g, ~0.5% ID/g, ~1% ID/g, and ~10% ID/g, respectively. Blocking with c(RGDyK) increased the intestinal radioactivity level to 16.57 ± 0.81% ID/g at 60 min. MicroPET imaging of 3.7 MBq (100 μCi) [^18^F]FBEM-SRGD was performed in nude mice bearing both the s.c. U87MG tumor and the orthotopic MDA-MB-435 tumor (1). The radioligand appeared to be excreted by both the liver and kidneys. There was also a fair amount of radioactivity in the abdomen up to 4 h. High radioactivity accumulation was observed in the tumor as early as 6 min. The liver and kidney radioactivity levels appeared to be much higher than that of the tumors.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(18F-RGD+OR+(18F-labeled+PEGylated+RGD+peptide))+AND+(dog+OR+rabbit+OR+pig+OR+sheep)&WebEnv=0lm4alv-2HCxC8e5RE3UcBkg5Er7OQct12zsixw-5BK4hv0paJj02SWyPp4qgQ9c2PBfpXFHkISyI%40D4664A2364)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(18F-RGD+OR+(18F-labeled+PEGylated+RGD+peptide))+AND+(primate+NOT+human)&WebEnv=0kkMh4y2inxOXWNkWiV0bqO0sAdEBRADMKKYVnn_Sr4yl6iKDVNKy2An4DI64c9iCSt2TXQ90s-TY%40D4664A2364C62360_0155S)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(18F-RGD+OR+(18F-labeled+PEGylated+RGD+peptide))+AND+human&WebEnv=0SffZNl7ihnQdRkfTQUS6M8Z4Nt545Ampfi4CXNXd3PL91KiaYZbG7pigmprTtZS6oBjCa9wGABOC%40D4664A2364C62360_0155SID&WebEnvRq=1)]

No publication is currently available.

## NIH Support

NIH CA93862, NCI P50 CA114747.

## References

1 Cai W., Zhang X., Wu Y., Chen X. (2006). A thiol-reactive 18F-labeling agent, N-[2-(4-18F-fluorobenzamido)ethyl]maleimide, and synthesis of RGD peptide-based tracer for PET imaging of alpha v beta 3 integrin expression. J Nucl Med.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Paulhe F., Manenti S., Ysebaert L., Betous R., Sultan P., Racaud-Sultan C. (2005). Integrin function and signaling as pharmacological targets in cardiovascular diseases and in cancer. Curr Pharm Des.
4 Hood J.D., Cheresh D.A. (2002). Role of integrins in cell invasion and migration. Nat Rev Cancer.
5 Hwang R., Varner J. (2004). The role of integrins in tumor angiogenesis. Hematol Oncol Clin North Am.
6 Cai W., Shin D.W., Chen K., Gheysens O., Cao Q., Wang S.X., Gambhir S.S., Chen X. (2006). Peptide-labeled near-infrared quantum dots for imaging tumor vasculature in living subjects. Nano Lett.
7 Massoud T.F., Gambhir S.S. (2003). Molecular imaging in living subjects: seeing fundamental biological processes in a new light. Genes Dev.
8 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
9 Chen X., Park R., Tohme M., Shahinian A.H., Bading J.R., Conti P.S. (2004). MicroPET and autoradiographic imaging of breast cancer alpha v-integrin expression using 18F- and 64Cu-labeled RGD peptide. Bioconjug Chem.
10 Chen X., Park R., Shahinian A.H., Tohme M., Khankaldyyan V., Bozorgzadeh M.H., Bading J.R., Moats R., Laug W.E., Conti P.S. (2004). 18F-labeled RGD peptide: initial evaluation for imaging brain tumor angiogenesis. Nucl Med Biol.
11 Chen X., Tohme M., Park R., Hou Y., Bading J.R., Conti P.S. (2004). Micro-PET imaging of alphavbeta3-integrin expression with 18F-labeled dimeric RGD peptide. Mol Imaging.
12 Chen X., Park R., Shahinian A.H., Bading J.R., Conti P.S. (2004). Pharmacokinetics and tumor retention of 125I-labeled RGD peptide are improved by PEGylation. Nucl Med Biol.
13 Chen X., Park R., Hou Y., Khankaldyyan V., Gonzales-Gomez I., Tohme M., Bading J.R., Laug W.E., Conti P.S. (2004). MicroPET imaging of brain tumor angiogenesis with 18F-labeled PEGylated RGD peptide. Eur J Nucl Med Mol Imaging.